# ^124^I-Labeled anti-prostate stem cell antigen affinity-matured A11 minibody

Chemical name: | ^124^I-Labeled anti-prostate stem cell antigen affinity-matured A11 minibody
Abbreviated name: | ^124^I-A11
Synonym: | ^124^I-Labeled A11 minibody
Agent Category: | Antibodies (minibodies)
Target: | Prostate stem cell antigen (PSCA)
Target Category: | Antigens
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^124^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=PSCA+and+antibody+fragments)]

The use of intact antibodies as molecular imaging agents has some disadvantages, such as large size, poor tumor penetration, and immunogenicity (1-4). To minimize these problems, various formats of antibody fragments have been designed with the variable regions of the light chain (V_L_) and the heavy chain (V_H_) (1, 5, 6). Monovalent single-chain Fv (scFv) constructs (molecular weight, 25–30 kDa) represent the smallest antibody fragments, which are generated with V_L_ and V_H_ connected by a flexible linker. Although monovalent scFv fragments exhibit efficient tumor penetration, they are cleared rapidly from blood and can demonstrate poor antigen binding. For example, the β half-life of monovalent scFv in plasma is only 0.5–2.0 h (in contrast to 48–72 h for intact antibodies) (1). Bivalent antibodies such as diabodies (molecular weight, 55–60 kDa) and minibodies (molecular weight, ~80 kDa) are ideal for tumor targeting because of their compact sizes and better antigen binding compared to monovalent scFv fragments (1, 7). Diabodies are dimeric molecules consisting of two scFv fragments connected with a short linker. Minibodies are formed by the fusion of scFv fragments with the immunoglobulin G1 (IgG1) C_H_3 domain. However, decreased antigen binding remains an issue for most antibody fragments compared with intact antibodies (1, 6, 8).

In previous studies, Olafsen et al. produced a humanized anti–prostate stem cell antigen (PSCA) intact antibody (hu1G8) and evaluated the antibody as an imaging agent (3). ^124^I-Labeled hu1G8 has been shown to specifically accumulate in LAPC-9 prostate tumor xenografts; however, it takes 1 week to reach the maximal tumor/background signal. To improve the antibody pharmacokinetics for imaging use, Leyton et al. engineered several antibody fragments on the basis of the hu1G8 sequence (7). The hu1G8 minibody (scFv-C_H_3 dimer; molecular weight, 80 kDa) is one of the fragments, and shows rapid blood clearance kinetics (MICAD chapter on ^124^I-anti-PSCA 2B3 (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Minibody2B3-124I) minibody). However, the apparent affinity of the hu1G8 minibody is only 5 nmol, representing a nine-fold loss compared with the apparent affinity of the intact hu1G8 antibody (46 nmol) (7). To increase the hu1G8 minibody affinity, Lepin et al. generated three affinity-matured minibody variants (A11, A2, and C5) with molecular evolution associated with yeast display, a powerful strategy for antibody affinity maturation (1). This strategy enables selection of scFv fragments with higher affinity from a yeast library generated with error-prone polymerase chain reaction (PCR). Lepin et al. demonstrated that the A11 variant has a higher affinity to PSCA than the parental hu1G8 minibody and exhibits more favorable pharmacokinetics for tumor imaging than other variants (1).

### Related Resource Links:

- MICAD chapters on PSCA-targeted agents (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=PSCA+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- MICAD chapters on antibody fragments (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=antibody+fragments+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information on human PSCA (http://www.ncbi.nlm.nih.gov/protein/?Db=gene&term=%28psca%5bgene%5d%29%20AND%20%28Homo%20sapiens%5borgn%5d%29%20AND%20alive%5bprop%5d%20NOT%20newentry%5bgene%5d&sort=weight)
- PSCA articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=PSCA)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=PSCA+and+hu1G8+antibody)]

Synthesis of the anti-PSCA mouse and human 1G8 intact antibodies and hu1G8 minibody has been reported previously and can be found in the MICAD chapter on ^124^I-anti-PSCA 2B3 (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Minibody2B3-124I) minibody as well (3, 6, 7, 9). Lepin et al. described the synthesis of the affinity-matured A11 minibody on the basis of the parental hu1G8 minibody (1). Briefly, the V_L_ and V_H_ coding sequences of the parental hu1G8 minibody were extracted and fused with an 18-residue GlySer-rich linker to form scFv in the V_L_–V_H_ orientation in the pYD2 expression vector. Random mutations were introduced into the scFv by error-prone PCR to construct a library of scFv variants on a yeast display. The library was subjected to four rounds of equilibrium-based selection. A11 was one of the three selected clones, possessing six mutations in the complementarity determining regions (CDRs): CDR 3 of V_L_ and CDR 2 of V_H_. The introduced mutations included a tyrosine, which is commonly used for iodination. To generate the A11 minibody, the A11 scFv variant sequences were fused to a signal peptide upstream and to the human IgG1 hinge and C_H_3 region downstream. Two million mouse myeloma cells were transfected, and clones were screened for expression. Soluble minibodies were purified from the cell culture supernatants with protein L chromatography. The best yield was 30 mg/l when expanded to terminal cultures into 2% fetal bovine serum (FBS). The purified minibody was radioiodinated with the Iodogen method. The labeling efficiency values were 89.9% and 86.6% for the parental hu1G8 and A11 minibodies, respectively. The molecular weight of each minibody was ~80 kDa, corresponding to a covalently linked minibody. The radiochemical purity and specific activity were not described.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=PSCA+and+hu1G8+antibody)]

The stability of A11 minibody was evaluated after 5 days incubation either at 4°C in phosphate-buffered saline (PBS) or at 37°C in 5% FBS. The activity showed a decrease of 12% and 13% in PBS and FBS, respectively, compared with frozen sample (1).

The affinity of the A11 minibody was tested against PSCA-mγ2a recombinant protein with non-labeled intact monoclonal antibody 1G8 as the competitor. The A11 minibody exhibited a higher affinity than the parental minibody (16 nmol versus 50 nmol). However, both minibodies showed lower affinity than the mouse monoclonal antibody 1G8.

The affinity of the A11 minibody was further tested with PSCA-transfected SKW6.4-PSCA (B-cell lymphoma) cells after incubation of the radioiodinated minibodies with an excess amount of cells for 1 h at room temperature. The immunoreactive fraction for the A11 minibody (66%) was significantly greater (P < 0.05) than that for the parental minibody (45%) (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=PSCA+and+hu1G8+antibody)]

Lepin et al. evaluated the A11 minibody for its biodistribution and its effectiveness in positron emission tomography (PET) imaging in mice bearing PSCA-expressing LAPC-9 human prostate tumors and Capan-1 human pancreatic tumors (1). The ^124^I-labeled minibodies were administered through the tail vein of mice. Thyroid uptake of radioiodine was blocked with Lugol administered with the minibodies. Stomach uptake of the radiolabeled minibodies was blocked with potassium perchlorate administered via gastric lavage 30 min before minibody injection.

In the LAPC-9 tumor model (n = 3 mice/group), the A11 minibody demonstrated better biodistribution and imaging results overall than the parental hu1G8 minibody. The kidney and liver uptakes were 1.3 ± 0.02% injected dose per gram tissue (ID/g) and 0.8 ± 0.04% ID/g, respectively, for ^124^I-A11, and 1.9 ± 0.41% and 1.3 ± 0.41% ID/g, respectively, for the parental minibody. Similar tumor uptake values were observed for both the A11 minibody (3.8 ± 0.27% ID/g) and the parental minibody (3.9 ± 0.26% ID/g) at 21 h after injection; however, a difference between them was observed for the tumor/blood ratio (1.1 versus 0.8) and for the tumor/background ratio (5.7 versus 2.4). The tumor imaging contrast was more than two-fold better with the A11 minibody than with the parental minibody.

Similar findings were obtained in the Capan-1 tumor model (n = 5 mice/group). The A11 minibody exhibited a slightly better tumor/blood ratio (0.96) than the parental minibody (0.8). A higher tumor/background ratio was reached with the A11 minibody (4.2) than with the parental minibody (2.2) (P < 0.001).

The investigators concluded that the ^124^I-A11 minibody is better than the parental minibody for PET imaging of PSCA-expressing tumors (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Lepin, E.J., J.V. Leyton, Y. Zhou, T. Olafsen, F.B. Salazar, K.E. McCabe, S. Hahm, J.D. Marks, R.E. Reiter, and A.M. Wu, An affinity matured minibody for PET imaging of prostate stem cell antigen (PSCA)-expressing tumors. Eur J Nucl Med Mol Imaging, 2010
2 Wu A.M. (2009). Antibodies and antimatter: the resurgence of immuno-PET. J Nucl Med.
3 Olafsen T., Gu Z., Sherman M.A., Leyton J.V., Witkosky M.E., Shively J.E., Raubitschek A.A., Morrison S.L., Wu A.M., Reiter R.E. (2007). Targeting, imaging, and therapy using a humanized antiprostate stem cell antigen (PSCA) antibody. J Immunother.
4 Wente M.N., Jain A., Kono E., Berberat P.O., Giese T., Reber H.A., Friess H., Buchler M.W., Reiter R.E., Hines O.J. (2005). Prostate stem cell antigen is a putative target for immunotherapy in pancreatic cancer. Pancreas.
5 Artiko V.M., Sobic-Saranovic D.P., Krivokapic Z.V., Petrovic M.N., Obradovic V.B. (2009). Is there a future role for immunoscintigraphy in the diagnosis of colorectal carcinoma?. Neoplasma.
6 Gu Z., Yamashiro J., Kono E., Reiter R.E. (2005). Anti-prostate stem cell antigen monoclonal antibody 1G8 induces cell death in vitro and inhibits tumor growth in vivo via a Fc-independent mechanism. Cancer Res.
7 Leyton J.V., Olafsen T., Lepin E.J., Hahm S., Bauer K.B., Reiter R.E., Wu A.M. (2008). Humanized radioiodinated minibody for imaging of prostate stem cell antigen-expressing tumors. Clin Cancer Res.
8 Saffran D.C., Raitano A.B., Hubert R.S., Witte O.N., Reiter R.E., Jakobovits A. (2001). Anti-PSCA mAbs inhibit tumor growth and metastasis formation and prolong the survival of mice bearing human prostate cancer xenografts. Proc Natl Acad Sci U S A.
9 Gu Z., Thomas G., Yamashiro J., Shintaku I.P., Dorey F., Raitano A., Witte O.N., Said J.W., Loda M., Reiter R.E. (2000). Prostate stem cell antigen (PSCA) expression increases with high gleason score, advanced stage and bone metastasis in prostate cancer. Oncogene.